# ^18^F-Labeled 4-(5-(2-(2-(2-fluoroethoxy)ethoxy)ethoxy)benzofuran-2-yl)-N,N-dimethylbenzenamine

Chemical name: | ^18^F-Labeled 4-(5-(2-(2-(2-fluoroethoxy)ethoxy)ethoxy)benzofuran-2-yl)-N,N-dimethylbenzenamine | [image]
Abbreviated name: | [^18^F]FPHBF-1 | [image]
Synonym: | [^18^F]17 | [image]
Agent Category: | Compounds | [image]
Target: | β-amyloid (Aβ) plaque | [image]
Target Category: | Accepters | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^18^F | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structures of benzofuran derivatives by Ono and Cheng et al. (1-3).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=molecular%20imaging%20and%20Alzheimer%u2019s%20disease%20and%20%u03B2-amyloid%20)]

^18^F-Labeled 4-(5-(2-(2-(2-fluoroethoxy)ethoxy)ethoxy)benzofuran-2-yl)-N,N-dimethylbenzenamine (FPHBF-1), abbreviated as [^18^F]FPHBF-1, is a fluoro-pegylated phenylbenzofuran synthesized for positron emission tomography (PET) of β-amyloid (Aβ) plaques by targeting Aβ (1-3).

Thioflavin T is a benzothiazole salt that is widely used to visualize and quantify the presence of Aβ in vitro (4, 5). Because of its high binding affinity with Aβ, thioflavin T has been intensively investigated as a template in the development of in vivo Aβ imaging agents (6-8). Ono et al. first synthesized a series of benzofuran derivatives by substituting N with CH on the heterocyclic ring of two thioflavin derivatives, TZDM (2-(4'-dimethylaminophenyl)-6-iodobenzothiazole) and IBOX (2-(4'-dimethylaminophenyl)-6-iodobenzoxazole) (4). Although these radioiodinated compounds displayed high binding affinity with Aβ in vitro with the inhibition constant (K_i_) values in the subnanomolar range and a brain uptake ranging from 0.5% to 1.5% initial dose/organ (at 2 min after injection), they suffered from slow clearance from the normal mouse brain (<50% at 2 h after injection) (4). The investigators then modified the structures of these benzofuran derivatives by substituting the methoxy group at the 5 position with hydroxy group (5). These derivatives showed considerable tolerance for structural modification in terms of binding affinity, and their clearance from the normal mouse brain markedly improved (5).

To further improve the pharmacokinetics of benzofuran derivatives, investigators synthesized fluoro-pegylated phenylbenzofuran FPHBF-1 and pyridylbenzofuran FPYBF-1 (1, 3). Both FPYBF-1 and FPHBF-1 possess a fluoropolyethylene glycol side chain and a dimethylaminopyridyl group. In healthy mice, FPYBF-1 displayed faster clearance than FPHBF-1 from the brain, which was explained by the lower lipophilicity of FPYBF-1. Because several imaging agents with a monomethylamino group (e.g., AV-45, BAY94-9172, and GE067) have been shown to be stable in vivo, and compounds with a monomethylamino group have a lower lipophilicity than the corresponding compounds with a dimethylamino group, Ono et al. generated N-monomethylated pyridylbenzofuran (FPYBF-2) and phenylbenzofuran (FPHBF-2) by replacing the dimethylaminopyridyl group in FPYBF-1 and FPHBF-1 with a monomethylamino group (2). FPYBF-2 and FPHBF-2 showed slightly less affinity than FPYBF-1 and FPHBF-1 but exhibited more favorable in vivo pharmacokinetics. These results further suggest that the introduction of further hydrophilic groups into the scaffold may lead to the development of more useful pyridylbenzofuran and phenylbenzofuran derivatives.

This chapter summarizes the data obtained with [^18^F]FPHBF-1. The data obtained with [^11^C]8 (http://www.ncbi.nlm.nih.gov/books/NBK23530/), [^18^F]FPYBF-1, [^18^F]FPYBF-2 (http://www.ncbi.nlm.nih.gov/books/NBK62347/), and [^18^F]FPHBF-2 (http://www.ncbi.nlm.nih.gov/books/NBK62346/) are summarized in other chapters on MICAD.

### Related Resource Links:

- Amyloid-targeted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=amyloid+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)
- Amyloid-targeted imaging clinical trials in ClinicalTrials.gov (http://clinicaltrials.gov/ct2/results?term=amyloid)
- Structures and other information of amyloid peptides in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance/?term=amyloid)
- Alzheimer’s disease articles in Online Mendelian Inheritance in Man (http://www.ncbi.nlm.nih.gov/omim/?term=Alzheimer%27s%20disease)

## Synthesis

[PubMed (http://pubs.acs.org/doi/abs/10.1021/ml100082x)]

Synthesis of the nonradiolabeled FPHBF-1 was described in detail by Cheng et al. (1). The key step in the formation of the benzofuran backbone was accomplished by an intramolecular Wittig reaction between triphenyl phosphonium salt and 4-nitrobenzoyl chloride or 4-dimethylaminobenzoyl chloride. [^18^F]FPHBF-1 was prepared from a tosyl precursor via a nucleophilic displacement reaction with a fluoride anion. For the final product, [^18^F]FPHBF-1, radiochemical yield was 10.0%, radiochemical purity was >99%, and specific activity was 242 GBq/μmol (6.54 Ci/µmol). The identity of [^18^F]FPHBF-1 was verified with a comparison of the retention time with the nonradioactive FPHBF-1.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://pubs.acs.org/doi/abs/10.1021/ml100082x)]

The affinity of nonradioactive FPHBF-1 with Aβ(1-42) peptide was measured in solutions with [^125^I]2-(4'-dimethylaminophenyl)-6-iodoimidazo[1,2-a]pyridine ([^125^I]IMPY, dissociation constant = 4.2 nM) as the competing radioligand (1, 9). The K_i_ values for FPYBF-1, FPHBF-1, FPYBF-2, FPHBF-2, and IMPY were 0.9, 2.0, 2.41, 3.85, and 10.5 nM, respectively (1-3). The calculated logarithms of water−octanol partition coefficients were 3.11, 3.73, 2.32, 2.94, and 3.79 for FPYBF-1, FPHBF-1, FPYBF-2, FPHBF-2, and IMPY, respectively (1-3).

To confirm the specific binding of [^18^F]FPHBF-1 to Aβ plaques, autoradiographic imaging of [^18^F]FPHBF-1 with sections (10 μm) of Tg2576 mouse brain was performed (1). The Tg2576 transgenic mice typically showed marked Aβ deposition in the cingulated cortex, entorhinal cortex, dentate gyrus, and CA1 hippocampal subfield by 11–13 months of age (1, 10). Autoradiographic images with [^18^F]FPHBF-1 showed high levels of radioactivity in the brain sections, which was confirmed for the Aβ plaque labeling with thioflavin-S staining.

## Animal Studies

### Rodents

[PubMed (http://pubs.acs.org/doi/abs/10.1021/ml100082x)]

The biodistribution of [^18^F]FPHBF-1 was analyzed in normal ddY male mice (n = 5/time point) (1). Mice were euthanized at 2, 10, 30, and 60 min after tail vein injection of 185–370 kBq (5–10 µCi). The radioactivity of the organs of interest was measured with a gamma counter. [^18^F]FPHBF-1 displayed high initial brain uptake (2.88% and 5.16% ID/g at 2 and 10 min after injection, respectively), and the radioactivity cleared with time (3.14% and 2.80% ID/g at 30 and 60 min after injection, respectively). The brain_2 min_/brain_60 min_ ratio (an index of washout rate) was 1.0, lower than that of agents [^18^F]BAY94-9172 (4.8), [^18^F]AV-45 (3.8), [^18^F]FPYBF-2 (2.34), [^18^F]FPHBF-2 (2.11), and [^18^F]FPYBF-1 (2.1), indicating a less favorable in vivo pharmacokinetics of [^18^F]FPHBF-1 (3, 11, 12). Uptake in the bone was 1.19% ID/g at 2 min and 2.74% ID/g at 60 min after injection, suggesting in vivo defluorination.

The potential of [^18^F]FPHBF-1 for imaging Aβ plaques in living brain tissue was examined in Tg2576 mice (36 months old, male) and in wild-type mice (36 months old, male) after tail vein injection of 9.29–11.1 MBq (0.25-0.3 mCi) [^18^F]FPHBF-1 (1). Animals were euthanized at 30 min after injection. Autoradiography ex vivo showed clear labeling of the Aβ plaques in the Tg2576 mouse brain, but not in the wild-type mouse brain. Aβ plaques were confirmed by co-staining the sections with thioflavin-S. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Cheng Y., et al. (2010). Fluorinated benzofuran derivatives for PET imaging of β-disease amyloid plaques in Alzheimer's disease brains. ACS Med Chem Lett.
2 Ono M., et al. (2011). Novel 18F-labeled benzofuran derivatives with improved properties for positron emission tomography (PET) imaging of beta-amyloid plaques in Alzheimer's brains. J Med Chem.
3 Cheng Y., et al. (2010). A novel 18F-labeled pyridyl benzofuran derivative for imaging of beta-amyloid plaques in Alzheimer's brains. Bioorg Med Chem Lett.
4 Ono M., et al. (2002). Benzofuran derivatives as Abeta-aggregate-specific imaging agents for Alzheimer's disease. Nucl Med Biol.
5 Ono M., et al. (2006). Novel benzofuran derivatives for PET imaging of beta-amyloid plaques in Alzheimer's disease brains. J Med Chem.
6 Mathis C.A., Wang Y., Klunk W.E. (2004). Imaging beta-amyloid plaques and neurofibrillary tangles in the aging human brain. Curr Pharm Des.
7 Ono M. (2009). Development of positron-emission tomography/single-photon emission computed tomography imaging probes for in vivo detection of beta-amyloid plaques in Alzheimer's brains. Chem Pharm Bull (Tokyo).
8 Vallabhajosula S. (2011). Positron emission tomography radiopharmaceuticals for imaging brain Beta-amyloid. Semin Nucl Med.
9 Newberg A.B., et al. (2006). Safety, biodistribution, and dosimetry of 123I-IMPY: a novel amyloid plaque-imaging agent for the diagnosis of Alzheimer's disease. J Nucl Med.
10 Hsiao K., et al. (1996). Correlative memory deficits, Abeta elevation, and amyloid plaques in transgenic mice. Science.
11 Zhang W., et al. (2007). 18F-labeled styrylpyridines as PET agents for amyloid plaque imaging. Nucl Med Biol.
12 Zhang W., et al. (2005). F-18 Polyethyleneglycol stilbenes as PET imaging agents targeting Abeta aggregates in the brain. Nucl Med Biol.